# Gd-Diethylenetriaminepentaacetic acid-polylysyl-N-glutaryl-phosphatidyl ethanolamine-2C5 liposomes

Chemical name: | Gd-Diethylenetriaminepentaacetic acid-polylysyl-N-glutaryl-phosphatidyl ethanolamine-2C5 liposomes
Abbreviated name: | Gd-DTPA-PLL-NGPE-2C5 liposomes
Synonym:
Agent category: | Antibody
Target: | Nucleosome-specific anti-nuclear autoantibodies (ANAs)
Target category: | Antigen
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Gadolinium (Gd)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd%202C5)]

Natural autoantibodies are produced when the immune system recognizes one or more of the body's normal constituents as foreign. These autoantibodies attack the body's own cells, tissues, or organs, leading to systemic autoimmune diseases. Nucleosome-specific anti-nuclear autoantibodies (ANAs) have been found to exhibit anti-tumor activity (1). The nucleosomes targeted by these antibodies are released from the dying tumor cells and bind to the adjacent healthy tumor cells, leading to the formation of ANAs specific to the nucleosomes (2). The nucleosome-specific ANA monoclonal antibody (mAb) 2C5 was found to have anti-tumor activity against a variety of experimental tumor models but showed no recognition of normal cells (1). There was an increased survival rate in cancer patients with elevated levels of serum ANAs (3, 4).

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (5, 6). Gd-Labeled diethylenetriaminepentaacetic acid (Gd-DTPA) was the first intravenous magnetic resonance imaging (MRI) contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and cancer. Furthermore, they are largely nonspecific. Investigators (7, 8) have prepared liposomes containing Gd-loaded polychelating polymers and the mAb 2C5 for MRI of ANA expression in nude mice bearing human cancer xenografts.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd%202C5+synthesis)]

Diethylenetriaminepentaacetic acid-polylysyl-N-glutaryl-phosphatidyl ethanolamine (DTPA-PLL-NGPE) (25 mg) was mixed with GdCl_3_ (37.5 mg) and incubated for 4 h at room temperature (7). Excess Gd ions were removed with dialysis. Gd-DTPA-PLL-NGPE polymers were ~30% Gd by weight. The liposomes were prepared by mixing egg phosphocholine, cholesterol, polyethylene glycol-phosphatidyl ethanolamine, and Gd-DTPA-PLL-NGPE in chloroform. After evaporation of chloroform, octyl glucoside in buffer saline (pH 7) was added to the film, and the mixture was mixed and sonicated for 1 h at 4°C. The liposomes were purified with dialysis. To prepare Gd-DTPA-PLL-NGPE-2C5 liposomes, micelles of PEG-PE-2C5 were incubated with Gd-DTPA-PLL-NGPE liposomes for 18 h. Gd-DTPA-PLL-NGPE-2C5 liposomes were purified with dialysis. Gd-DTPA-PLL-NGPE-2C5 liposomes had an average size of 152 nm and contained ~16 mM phospholipids. Neither the number of DTPAs per mAb nor 2C5 mAbs per liposome was reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd%202C5+in+vitro)]

Gd-DTPA-PLL-NGPE liposomes exhibited R_1_ relaxivity rates (5 MHz) of 0.065 ± 0.006 ms compared with 0.003 ± 0.001 ms for Gd-DTPA-PE liposomes measured at room temperature in saline (pH 7.4) (7). Gd-DTPA-PLL-NGPE-2C5 liposomes and 2C5 mAbs exhibited similar immunoreactivity for immobilized nucleosomes. Gd-DTPA-PLL-NGPE-2C5 liposomes exhibited R1 relaxivity rates approximately twice that of Gd-DTPA-PLL-NGPE liposomes and Gd-DTPA-PLL-NGPE-IgG liposomes as measured in three cancer cell lines (LLC, BT-20, and MCF-7). Chakilam et al. (9) showed that the binding affinity (K_d_) of 2C5 mAb for nucleosomes was 0.24 ± 0.06 nM. Flow cytometry analyses confirmed 2C5 mAb binding to eight broad variety human tumor cell lines (COLO-205, PC-3, C32TG, NCI-H82, MCF7, H9, H69 AR, and BT-20).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd%202C5+rodentia)]

Erdogan et al. (8) performed 9.4-T MRI studies in mice bearing human LLC tumor xenografts with Gd-DTPA-PLL-NGPE-2C5 liposomes and Gd-DTPA-PLL-NGPE liposomes. There was a significant increase (P < 0.05–0.01) in tumor R_1_ values for Gd-DTPA-PLL-NGPE-2C5 liposomes over R_1_ values for Gd-DTPA-PLL-NGPE liposomes at 4, 24, and 48 h after injection. Gd-DTPA-PLL-NGPE-IgG liposomes showed tumor R_1_ values similar to those of Gd-DTPA-PLL-NGPE liposomes. Confocal microscopy and ex vivo MRI studies confirmed the localization of only Gd-DTPA-PLL-NGPE-2C5 liposomes to the surface of the LLC tumor cells and not to normal muscle cells. No blocking experiment was performed. Did Gd-DTPA-PLL-NGPE bind to tumor or normal cells? That would suggest some selectivity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%202C5+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%202C5+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+2C5+human)]

No publication is currently available.

## NIH support

R01 EB02995

## References

1 Iakoubov L.Z., Torchilin V.P. (1997). A novel class of antitumor antibodies: nucleosome-restricted antinuclear autoantibodies (ANA) from healthy aged nonautoimmune mice. Oncol Res.
2 Iakoubov L.Z., Torchilin V.P. (1998). Nucleosome-releasing treatment makes surviving tumor cells better targets for nucleosome-specific anticancer antibodies. Cancer Detect Prev.
3 Blaes F., Klotz M., Huwer H., Straub U., Kalweit G., Schimrigk K., Schafers H.J. (2000). Antineural and antinuclear autoantibodies are of prognostic relevance in non-small cell lung cancer. Ann Thorac Surg.
4 Syrigos K.N., Charalambopoulos A., Pliarchopoulou K., Varsamidakis N., Machairas A., Mandrekas D. (2000). The prognostic significance of autoantibodies against dsDNA in patients with colorectal adenocarcinoma. Anticancer Res.
5 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
6 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
7 Erdogan S., Roby A., Sawant R., Hurley J., Torchilin V.P. (2006). Gadolinium-loaded polychelating polymer-containing cancer cell-specific immunoliposomes. J Liposome Res.
8 Erdogan S., Medarova Z.O., Roby A., Moore A., Torchilin V.P. (2008). Enhanced tumor MR imaging with gadolinium-loaded polychelating polymer-containing tumor-targeted liposomes. J Magn Reson Imaging.
9 Chakilam A.R., Pabba S., Mongayt D., Iakoubov L.Z., Torchilin V.P. (2004). A single monoclonal antinuclear autoantibody with nucleosome-restricted specificity inhibits growth of diverse human tumors in nude mice. Cancer Therapy.